# Ethyl-3,5-bis(acetylamino)-2,4,6-triiodobenzoate nanoparticles

Chemical name: | Ethyl-3,5-bis(acetylamino)-2,4,6-triiodobenzoate nanoparticles
Abbreviated name: | N1177
Synonym:
Agent Category: | Triiodobenzoate
Target: | Macrophages
Target Category: | Phagocytosis
Method of detection: | X-ray computed tomography (CT)
Source of signal/contrast: | Iodine
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=N1177)]

Macrophages are key cellular mediators of inflammation in atheroma and participate in all stages in evolving atherosclerotic plaques (1, 2). The atheroma lesion is normally initialized by recruiting monocytes in inflamed intima. Monocytes mature into macrophages under the in situ stimulation of overexpressed macrophage colony-stimulating factor. As cholesteryl esters gradually accumulate in cytoplasm, macrophages are converted into foam cells at the early stage of atheroma. The accumulation of foam cells leads to the formation of fatty streaks and the deposition of fibrous tissues, which indicates the progression of atheroma into an intermediate stage. Fibrous caps are formed on the surface of a lipid-rich core and result in vulnerable atherosclerotic plaque as the smooth muscle cells synthesize bulk extracellular matrix. Finally, the rupture of the atherosclerotic plaques and the calcification of vessel walls progressively occlude the lumen. The vulnerable plaques are considered as a “high-risk” stage, which contain much higher levels of macrophages than that in any other stage (3). Thus, measuring macrophage density in plaques becomes an alternative approach to evaluate the vulnerable plaques (4). Atherosclerotic plaques can be generated in rabbits by balloon injury in the aortas followed by hypercholesterolemic diet (4). This animal model provides high levels of macrophages with sizes similar to those found in the human coronary atherosclerotic plaques, suitable for examining the effects of antiatherosclerotic drugs on atherosclerotic plaque size and composition.

Multi-detector row computed tomography (MDCT) has been used as a robust imaging modality for non-invasive assessment of coronary arteries (5, 6). In particular, the development of 64-slice MDCT (64-MDCT) provides fast gantry rotation time (0.33 s) and small imaging voxel size (0.4 mm^3^) (7), which allows for reliable assessment of atherosclerotic plaques (8). Because their CT attenuation differences are much larger than 30 HU (a criteria in delineation of tissues), calcified plaques (391–419 HU), fibrous plaques (70–104 HU), and lipid-rich plaques (soft plaques, 14–49 HU) can be directly differentiated with the use of MDCT (8). To measure the macrophage density in the plaques requires a macrophage-specified CT contrast agent (4). Iodinated compounds have been used as CT contrast agents for many years. Small molecules such as iopamidol can attenuate the X-ray density up to 30 HU at a dosage of 1 mg iodine/g tissue (9), but they are not specific imaging agents for macrophages. Contrast agents can be incorporated into macrophages through phagocytosis, a special macrophage uptake process. Sparingly soluble crystals, supramolecular aggregates, large micelles, or emulsions of iodinated lipids are suitable for this purpose. All of these contrast agents should have a sufficiently large size to be marked (“opsonized”) by circulating proteins (“opsonins”), then followed by phagocytosis (9). Ethyl-3,5-bis(acetylamino)-2,4,6-triiodobenzoate nanoparticles (N1177) is an emulsified suspension that is composed of crystalline iodinated particles dispersed with surfactant (4). The iodinated particles, ethyl-3,5-bis(acetylamino)-2,4,6-triiodobenzoate, are an esterified derivative of the X-ray contrast agent diatrizoic acid with a very low aqueous solubility (~2 μg/ml). Two biocompatible surfactants, a polyoxyethylene-polyoxypropylene block co-polymer (poloxamer 338) and a polyethylene glycol, are added to stabilize the particles and prevent aggregation.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(N1177)+AND+synthesis%0D%0A)]

Hyafil et al. reported the detailed synthesis of N1177 (4). Initially, 6-ethoxy-6-oxohexy-3,4-bis(acetylamino)-2,4-triiodobenzoate (C_19_H_23_I_3_N_2_O_6_), also called iodinated aroyloxy ester, was obtained by condensation of 6-bromohexanoate with sodium diatrizoate in dimethyl formamide followed by precipitation in dimethyl sulfoxide. The produced iodinated aroyloxy ester was milled with poloxamer 338 in the presence of inert beads to generate a nanoparticulate suspension, which was separated from the beads by membrane filtration with membrane pore diameter of 2–5 μm. Then, polyethylene glycol 1450 and tromethamine were added to the obtained suspension to stabilize the particles and to maintain a neutral pH. The final product (N1177) was composed of 150 mg/ml of iodinated aroyloxy ester, 30 mg/ml of poloxamer 338, 150 mg/ml of polyethylene glycol 1450, and 0.36 mg of tromethamine, and remained stable for ~8 months. The size of N1177 particle ranged from 153 nm to 408 nm with a mean value of 259 nm. Transmission electron microscopy of N1177 demonstrated that cores formed by electron-dense granules were covered by molecular polymers, and iodine was present in the electron-dense granules.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(N1177)+AND+%22in+vitro%22)]

Hyafil et al. examined the in vitro uptake of N1177 in mouse macrophages (4). After incubation with N1177 (n = 6 mice) or iopamidol (n = 6 mice) as control for 1 h, numerous dark granules were observed in the cytoplasm of macrophages that were incubated with N1177. The cell-internalized iodine was quantified with inductively coupled plasma mass spectrometry, which revealed a substantially higher uptake of N11777 by macrophages as compared to uptake by iopamidol (4,920 ± 1,019 versus 56 ± 11 μg iodine/g cell pellets).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(N1177) +AND++rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

The pharmacokinetics of N1177 was measured in healthy rabbits (4). After rabbits (n = 8) intravenous injections of N1177 at a dose of 250 mg iodine/kg, a series of CT images were collected to examine the enhancement in the blood and in macrophage-rich tissues. At 5 minutes after injection, the X-ray absorption value was found to be 125.3 ± 14.1 HU in the aortic lumen. This enhancement allowed for clear delineation of all major arterial and venous contours by CT. Two hours after injection of N1177, the vascular enhancement of N1177 was decreased rapidly, i.e., the absorption value measured in the aortic lumen returned to its precontrast level (42.3 ± 3.7 HU), whereas the enhancement in macrophage-rich tissues such as spleen and liver was significantly higher than that of precontrast level: 106.7 ± 6.5 versus 65.2 ± 2.2 HU in the spleen, and 114.4 ± 10.3 versus 63.1 ± 5.1 HU in the liver. No CT enhancement was found in other macrophage-deficient organs, such as muscles. A low enhancement in kidneys and in the urinary tract 1 h after injection of N1177 was caused by the renal excretion of N1177. No residual enhancement was detectable 24 h after the injection of N1177. As a control, the same rabbit was imaged 1 week later, followed by injection of iopamidol at 250 mg iodine/kg. The X-ray absorption value was much lower, 61.8 ± 13.9 HU at 5 min after injection of iopamidol. No enhancement was found in spleen and liver 2 h later.

The in vivo uptake of N1177 in macrophages was examined in atherosclerotic plaques in rabbits (n = 8) (4). The atherosclerotic plaques were generated by double balloon injuries in the aortas within one month’s time, followed by 4 months of hypercholesterolemic diet. Healthy rabbits (n = 4) with a chow diet were used as control. All rabbits were first imaged with 64-MDCT after injection of iopamidol, and they were imaged again 1 week later after injection of N1177 at a dose of 250 mg iodine/kg. All CT images were collected at 2 h after injection, when enhancement of macrophage-rich tissues reached the highest value and the enhancement in the aortic lumen decreased to nearly zero, which allowed for clear discrimination between the macrophage-rich atherosclerotic plaques and the aortic lumen in the images. The enhancement in atherosclerotic plaques was 13.3 ± 1.0 HU for N1177 and 4.1 ± 0.9 HU for iopamidol. For the control rabbits, no substantial enhancement was found in the arterial wall at 2 h after injection of N1177 (0.9 ± 1.2 HU) or iopamidol (0.3 ± 1.3 HU). After the imaging experiment, the aortas were excised for histological analysis of fibrous caps and lipid-rich cores in the atherosclerotic plaques. The results exhibited a correlation between the enhancement of N1177 on the CT image at 2 h and the intensity of macrophage infiltration in the corresponding histological section. A CT contrast enhancement ≥13.3 HU corresponded to a macrophage area extending to >20% of the intimal area. No macrophage was found in the aortic wall of control rabbits. Transmission electron microscopy demonstrated the presence of a large number of electron-dense granules in the lysosomes of macrophages in the atherosclerotic plaques of the excised tissues. Energy dispersion spectrometry confirmed that these granules showed contained iodine caused by the accumulation of N1177 in macrophages of atherosclerotic plaques.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(N1177) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(N1177) +AND+human)]

No publication is currently available.

### NIH Support

HL 71021, HL 78667

## References

1 Jaffer F.A., Libby P., Weissleder R. (2006). Molecular and cellular imaging of atherosclerosis: emerging applications. J Am Coll Cardiol.
2 Packard R.R., Libby P. (2008). Inflammation in atherosclerosis: from vascular biology to biomarker discovery and risk prediction. Clin Chem.
3 Yan Z.Q., Hansson G.K. (2007). Innate immunity, macrophage activation, and atherosclerosis. Immunol Rev.
4 Hyafil F., Cornily J.C., Feig J.E., Gordon R., Vucic E., Amirbekian V., Fisher E.A., Fuster V., Feldman L.J., Fayad Z.A. (2007). Noninvasive detection of macrophages using a nanoparticulate contrast agent for computed tomography. Nat Med.
5 Schmid M., Pflederer T., Jang I.K., Ropers D., Sei K., Daniel W.G., Achenbach S. (2008). Relationship between degree of remodeling and CT attenuation of plaque in coronary atherosclerotic lesions: an in-vivo analysis by multi-detector computed tomography. Atherosclerosis.
6 Schroeder S., Kopp A.F., Burgstahler C. (2007). Noninvasive plaque imaging using multislice detector spiral computed tomography. Semin Thromb Hemost.
7 Flohr T.G., McCollough C.H., Bruder H., Petersilka M., Gruber K., Suss C., Grasruck M., Stierstorfer K., Krauss B., Raupach R., Primak A.N., Kuttner A., Achenbach S., Becker C., Kopp A., Ohnesorge B.M. (2006). First performance evaluation of a dual-source CT (DSCT) system. Eur Radiol.
8 Pohle K., Achenbach S., Macneill B., Ropers D., Ferencik M., Moselewski F., Hoffmann U., Brady T.J., Jang I.K., Daniel W.G. (2007). Characterization of non-calcified coronary atherosclerotic plaque by multi-detector row CT: comparison to IVUS. Atherosclerosis.
9 Krause W. (1999). Delivery of diagnostic agents in computed tomography. Adv Drug Deliv Rev.